# (S)-2-Amino-3-[1-(2-[^18^F]fluoroethyl)-1H-[1,2,3]triazol-4-yl]propanoic acid

Chemical name: | (S)-2-Amino-3-[1-(2-[^18^F]fluoroethyl)-1H-[1,2,3]triazol-4-yl]propanoic acid
Abbreviated name: | (S)-[^18^F]4
Synonym:
Agent category: | Compound
Target: | Cationic amino acid transporter, L-type amino acid transporter
Target category: | Transporter
Method of detection: | Positron emission tomography
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids compared with uptake in normal brain tissue (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used for imaging in oncology, although no radiolabeled amino acid is approved in the US at present (1, 4, 5).

More than twenty amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and the Na-dependent transporter system A, as well as through the Na^+^-dependent system B^0^ (6). The amino acids are retained in tumor cells, including incorporation into proteins, due to their high metabolic activities, which are higher than metabolic activities of most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells were found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6), but they are not approved by the United States Food and Drug Administration. These radiolabels are moved into cells by various amino acid transporters and are incorporated into proteins, although only L-leucine is quantitatively incorporated into proteins. The fraction of radiolabeled amino acids that is incorporated into proteins is usually small compared to the total amount taken up into the cell. Imaging techniques that use natural amino acids are based on amino acid transport and protein incorporation.

Non-natural amino acids are not incorporated into proteins (2, 8); instead, they are rapidly transported into tumor cells. They are retained inside the tumor cells because of their high cellular metabolism and the high activity of the amino acid transporters. A new L-tyrosine analog, O-(2-[^18^F]fluoroethyl)-L-tyrosine ([^18^F]FET), has been synthesized and evaluated as an amino acid PET tracer for the detection of brain tumors. [^18^F]FET has a higher specificity than [^18^F]FDG (8). (S)-2-Amino-3-[1-(2-[^18^F]fluoroethyl)-1H-[1,2,3]triazol-4-yl]propanoic acid ((S)-[^18^F]4) has been found to be a substrate for the cationic amino acid transporter, which transports the naturally occurring amino acids (L-histidine, L-arginine, and L-lysine) (9). (S)-[^18^F]4 was synthesized with Click reaction and evaluated as an amino acid PET tracer for the detection of brain tumors.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (Cationic amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/84889), L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20synthesis)]

McConathy et al. (9) reported the synthesis of (S)-[^18^F]4 in a multi-step reaction. 2-[^18^F]Fluoroethyl azide was prepared using the tosylate (S)-precursor in the presence of K[^18^F]F/K2.2.2/K_2_CO_3_ (85°C, 15 min). Cycloaddition reaction of 2-[^18^F]fluoroethyl azide to the alkyne precursor was carried out in N,N-dimethylformamide for 15 min at room temperature. The purified reaction product was subjected to acid hydrolysis to form (S)-[^18^F]4. (R)-[^18^F]4 was prepared similarly using the tosylate (R)-precursor. (S)-[^18^F]4 and (R)-[^18^F]4 were obtained with radiochemical yields of 51 ± 8% (n = 5) and 57 ± 6% (n = 3), respectively. The radiochemical purity was >98% with a total synthesis time of ~150 min. The specific activities for (S)-[^18^F]4 and (R)-[^18^F]4 were 37 and 11 GBq/µmol (1 and 0.3 Ci/µmol) at the time of biological studies, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20in%20vitro)]

McConathy et al. (9) showed that (S)-[^18^F]4 accumulation in 9L rat gliosarcoma cells was reduced by 50%, 18%, and 89% in the presence of 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (BCH, an L-type transporter inhibitor), N-methyl-α-aminoisobutyric acid (an A-type transporter inhibitor), and L-alanine/serine/cysteine (ASC, control), respectively. The further inhibition of uptake by BCH under sodium-free conditions suggests (S)-[^18^F]4 is a substrate for system L transport. (S)-[^18^F]4 accumulation in cells was inhibited by 50% with L-Arg and by 69% with L-His, suggesting involvement of cationic amino acid transport. In contrast, (R)-[^18^F]4 accumulation was not mediated by system L or by cationic amino acid transport. (R)-[^18^F]4 accumulation was only partially inhibited (36%) by ASC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20rodentia)]

The biodistribution of (S)-[^18^F]4 and (R)-[^18^F]4 (1.1–1.9 MBq (0.03–0.5 mCi)) was studied in rats bearing subcutaneous 9L gliosarcoma tumors (n = 3–4/group) at 15, 30, and 60 min after injection (9). (S)-[^18^F]4 and (R)-[^18^F]4 showed similar accumulation (percent injected dose/gram (% ID/g)) in most normal tissues with the exception of the pancreas and spleen, where (S)-[^18^F]4 showed higher accumulation than (R)-[^18^F]4. Tumor accumulation of (S)-[^18^F]4 was 0.47%, 0.83%, and 0.72% ID/g at 15, 30, and 60 min, respectively. Tumor accumulation of (R)-[^18^F]4 was 0.27%, 0.29%, and 0.17% ID/g at 15, 30, and 60 min, respectively. High accumulation was observed in the pancreas (2.75% ID/g, 0.53% ID/g), lung (0.87% ID/g, 0.74% ID/g), and kidney (11.0% ID/g, 14.0% ID/g) for (S)-[^18^F]4 and (R)-[^18^F]4, respectively, at 15 min after injection. The radioactivity level in the bone declined over the 60-min period, indicating little defluorination. The tumor/blood ratios of (S)-[^18^F]4 (1.8, 3.2) at 30 min and 60 min, respectively, were higher than those of (R)-[^18^F]4 (1.0, 1.2) at the same time points. Accumulation of both tracers was low in the brain. The tumor/brain ratios at 60 min after injection were 15.2 and 6.9 for (S)-[^18^F]4 and (R)-[^18^F]4, respectively. No blocking experiment was performed.

PET imaging scans were performed with ~10 MBq (0.27 mCi) (S)-[^18^F]4 over 120 min after injection in rats with subcutaneous (n = 2) and intracranial (n = 1) 9L gliosarcoma tumors. Both tumors showed rapid tumor accumulation at 5 min and reached a plateau at ~30 min. High radioactivity levels were observed in the kidneys and urinary bladder. The subcutaneous tumor/muscle ratio was ~6 at 30 min, and the intracranial tumor/brain ratio was ~7 at the same time point. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20triazol%20propanoic%20acid%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
9 McConathy J., Zhou D., Shockley S.E., Jones L.A., Griffin E.A., Lee H., Adams S.J., Mach R.H. (2010). Click synthesis and biologic evaluation of (R)- and (S)-2-amino-3-[1-(2-[18F]fluoroethyl)-1H-[1,2,3]triazol-4-yl]propanoic acid for brain tumor imaging with positron emission tomography. Mol Imaging.